# [^11^C]Methylated LY2181308

Chemical name: | [^11^C]Methylated LY2181308
Abbreviated name: | [^11^C]LY2181308
Synonym:
Agent category: | Oligonucleotide
Target: | Survivin
Target category: | Ribonucleic acid (RNA)
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=LY2181308)]

Survivin is a small protein (142 amino acids, 16.5 kDa) that belongs to the inhibitor of apoptosis protein (IAP) family (1). IAPs can effectively suppress apoptosis induced by a variety of stimuli, including death receptor activation, growth factor withdrawal, ionizing radiation, viral infection, and genotoxic damage. Survivin comprises a single baculovirus IAP repeat domain and an extended COOH-terminal α-helical coiled-coil domain but lacks the RING-finger domain found in other IAPs. In addition to suppressing apoptosis, survivin is involved in many essential cellular functions, such as cell division, cell stress response, and surveillance checkpoints. Survivin is strongly expressed in the majority of human tumor types (2). As a new target in cancer treatment, inhibition of survivin expression can be carried out through the use of anti-sense oligonucleotides, ribozymes, and small interfering RNA (3). LY2181308 is an 18-mer survivin anti-sense oligonucleotide (6.8 kDa) against survivin mRNA (4, 5). Dence et al. (6) developed a rapid method for randomly ^11^C-methylated LY2181308 ([^11^C]LY2181308) for positron emission tomography (PET) imaging of survivin mRNA expression in tumors.

### Related Resource Links:

- Chapters in MICAD (Survivin (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Survivin%20AND+micad%5Bbook%5D))
- Gene information in NCBI (Survivin (http://www.ncbi.nlm.nih.gov/gene/332))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Survivin (http://www.ncbi.nlm.nih.gov/omim/603352))
- Clinical trials (LY2181308 (http://www.clinicaltrials.gov/ct2/results?term=ly2181308))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=LY2181308%20and%20synthesis)]

Dence et al. (6) reported the synthesis of [^11^C]LY2181308 by ^11^C-methylation of LY2181308 with [^11^C]iodomethane in the presence of sodium borate in dimethylformamide for 3 min at 90ºC. [^11^C]LY2181308 was purified with column chromatography. The specific activity of [^11^C]LY2181308 was 22.2 GBq/μmol (600 mCi/μmol), with >97% radiochemical purity and an average radiochemical yield of 43 ± 15% (decay-corrected, n = 5) at the end of bombardment. The total synthesis time was 40–45 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=LY2181308%20and%20in%20vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=LY2181308%20and%20rodentia)]

Dence et al. (6) reported ex vivo biodistribution studies of 3.7 MBq (0.1 mCi) [^11^C]LY2181308 in mice (n = 3 mice/group) bearing EMT-6 mouse breast tumors. Radioactivity accumulation was measured at 5, 30, and 60 min after injection. The highest accumulation of radioactivity at 30 min was found in the kidney (72.4% injected dose/gram (ID/g)), followed by the liver (26.6% ID/g), spleen (6.9% ID/g), and lung (2.6% ID/g). The accumulation was <2.2% ID/g in the thymus, heart, muscle, and blood. The accumulation in the tumors was 2.09 ± 0.32% ID/g, 2.89 ± 0.67% ID/g, and 2.61 ± 0.93% ID/g at 5, 30, and 60 min, respectively. The blood radioactivity level was 0.6% ID/g at 60 min. Co-injection of LY2181308 (~7.5 nmol) reduced the accumulation in the kidney, liver, and spleen by 35%, 44%, and 23%, respectively, at 60 min after injection. These results are consistent with the expression of survivin mRNA in these normal organs. On the other hand, co-injection of LY2181308 increased accumulation in the tumor by 39% at 60 min after injection. The authors suggested that the dose of LY2181308 was not sufficient in vivo to block [^11^C]LY2181308 accumulation in the tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=LY2181308%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=LY2181308%20and%20%28primate%20not%20human%29)]

Dence et al. (6) reported whole-body PET imaging in one male and two female baboons to estimate human dosimetry after injection of 290 MBq (7.9 mCi) [^11^C]LY2181308. The kidney had the highest radiation dose of 32 µGy/MBq (118 mrad/mCi), followed by the liver with 22 µGy/MBq (82 mrad/mCi) and the heart wall with 8 µGy/MBq (29 mrad/mCi). All other organs had <6 µGy/MBq (20 mrad/mCi). The effective dose equivalent was 8.8 µSv/MBq (25.3 mrem/mCi).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=LY2181308%20and%20human)]

No publication is currently available.

## References

1 Pennati M., Folini M., Zaffaroni N. (2008). Targeting survivin in cancer therapy. Expert Opin Ther Targets.
2 Zaffaroni N., Pennati M., Daidone M.G. (2005). Survivin as a target for new anticancer interventions. J Cell Mol Med.
3 Ryan B.M., O'Donovan N., Duffy M.J. (2009). Survivin: a new target for anti-cancer therapy. Cancer Treat Rev.
4 Carrasco, R.A., N.B. Stamm, E.G. Marcusson, G.E. Sandusky, P. Iversen, and B.K. Patel, Antisense Inhibition of Survivin Expression as a Cancer Therapeutic. Mol Cancer Ther, 2011
5 Rodel F., Frey B., Leitmann W., Capalbo G., Weiss C., Rodel C. (2008). Survivin antisense oligonucleotides effectively radiosensitize colorectal cancer cells in both tissue culture and murine xenograft models. Int J Radiat Oncol Biol Phys.
6 Dence C.S., Laforest R., Sun X., Sharp T.L., Welch M.J., Mach R.H. (2010). Radiochemical synthesis, rodent biodistribution and tumor uptake, and dosimetry calculations of [(1)(1)C] methylated LY2181308. Mol Imaging Biol.